# ^64^Cu-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_
Abbreviated name: | ^64^Cu-NODAGA-LM3
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor 2 (SSTR2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SST receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (SSTR1–SSTR5) have been identified and subsequently cloned from animal and human tissues (3, 4). SSTR also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-Diethylenetriamine pentaacetic acid-octreotide (^111^In-DTPA-OCT) is an SST analog that, over the last decade, has remained the most widely used radiopharmaceutical and the only FDA approved radiotracer for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs with single-photon emission computed tomography (SPECT) (6). It has also shown promising results in peptide-receptor radionuclide therapy (7). Octreotide (OCT) is a cyclic peptide with eight amino acids. ^111^In-DTPA-OCT binds with high affinity to SSTR2 and SSTR5 and to SSTR3 to a lesser degree, but it does not bind to SSTR1 and SSTR4 (8). A large number of radiolabeled SST analogs have been reported using different radionuclides and different linkers. Currently used targeting SSTR peptides are mainly SSTR2 agonists. Therefore, there is a need for SSTR2 antagonist radioligands (9). p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_ (LM3) is a novel selective SSTR2 antagonist. Fani et al. (10) prepared ^64^Cu-1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid-LM3 (^64^Cu-NODAGA-LM3) as a positron emission tomography (PET) imaging agent for SSTR2.

### Related Resource Links:

- Chapters in MICAD (Somatostatin (http://www.ncbi.nlm.nih.gov/books?term=Somatostatin%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Somatostatin (http://www.ncbi.nlm.nih.gov/gene/6750), SSTR2 (http://www.ncbi.nlm.nih.gov/gene/6752))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Somatostatin (http://omim.org/entry/182450), SSTR2 (http://omim.org/entry/182452))
- Clinical trials (Somatostatin receptor (http://www.clinicaltrials.gov/ct2/results?term=somatostatin+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+synthesis)]

NODAGA-LM3 was synthesized via standard solid-phase peptide synthesis with a calculated mass of 1,522.6 Da in agreement with mass spectrometry (10). NODAGA was incorporated at the N-terminus of the peptide. NODAGA-LM3 was purified with high-performance liquid chromatography. ^64^Cu was complexed to NODAGA-LM3 by reaction of 3.3 nmol NODAGA-LM3 with 37 MBq (1 mCi) ^64^CuCl_2_ in ammonium acetate (pH 8.0) for 10 min at room temperature. ^64^Cu-NODAGA-LM3 had a >95% radiochemical purity and specific activity of 20 MBq/nmol (0.54 mCi/nmol), with a labeling yield >97%. ^64^Cu-NODAGA-LM3 had a log D value of –2.02 ± 0.01 and a net charge of zero.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+in+vitro)]

Fani et al. (10) reported that ^nat^Cu-NODAGA-LM3 had 50% inhibition concentration (IC_50_) values of >1,000, 6.7 ± 1.5, >1,000, >1,000, and >1,000 nM for human SSTR1, SSTR2, SSTR3, SSTR4, and SSTR5 receptors in competition with ^125^I-SRIF-28, respectively. ^64^Cu-NODAGA-LM3 bound to the cell surface of HEK-sst2 cells with ~30% of the incubation dose at 30 min and ~40% incubation dose at 4 h. Internalization of ^64^Cu-NODAGA-LM3 was ~12% and was inhibited to 1% incubation dose with excess unlabeled ligand. After 4 h in fresh medium, 55% of radioactivity remained on the cell surface, 16% was internalized, and 26% was found in the medium. Immunofluorescence studies showed that [Tyr^3^]octreotide (10 nM) triggers receptor internalization whereas ^nat^Ga-NODAGA-LM3 at a much higher concentration (1,000 nM) does not stimulate receptor internalization in HEK-sst2 cells. ^nat^Cu-NODAGA-LM3 was able to inhibit receptor internalization induced by [Tyr^3^]octreotide.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+rodentia)]

Fani et al. (10) performed ex vivo biodistribution studies with 5.55 MBq (0.15 mCi) ^64^Cu-NODAGA-LM3 in nude mice (n = 3–7/group) bearing HEK-sst2 xenografts at 1, 4, and 24 h after injection. The accumulation of radioactivity in the SSTR2 tumor was 35.46 ± 5.70% injected dose per gram (% ID/g) at 1 h, 37.88% ID/g at 4 h, and 14.79% ID/g at 24 h after injection. The pancreas had the highest accumulation (16.26% ID/g) at 1 h after injection, followed by the kidney (10.90% ID/g), stomach (9.17% ID/g), lung (5.89% ID/g), and liver (2.23% ID/g). Accumulation of radioactivity in the other tissues was low. The concentration in the blood was 0.11% ID/g at 4 h after injection, with tumor/blood ratios of 42, 344, and 123 at 1, 4, and 24 h, respectively. Co-injection with 2,000-fold excess DOTA-LM3 reduced the accumulation of radioactivity by 98% in the tumor, 67% in the stomach, and 78% in the pancreas at 4 h after injection (all known to contain SSTR). Little or no inhibition was observed in the other tissues. In comparison, ^64^Cu-NODAGA-LM3 accumulation in the kidney was 1-, 3-, and 8- fold lower than that of ^64^Cu-CB-TE2A-LM3 at 1, 4, and 24 h, respectively. The tumor/tissue ratios (blood, kidney, liver, and muscle) were significantly higher for ^64^Cu-NODAGA-LM3 than for ^64^Cu-CB-TE2A-LM3 (P < 0.01).

Whole-body PET imaging visualized the SSTR2 tumor at 4 h and 24 h after injection of 6 MBq (0.16 mCi) ^64^Cu-NODAGA-LM3 (n=1). No blocking studies were carried out.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+human)]

No publication is currently available.

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
8 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
9 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
10 Fani M., Del Pozzo L., Abiraj K., Mansi R., Tamma M.L., Cescato R., Waser B., Weber W.A., Reubi J.C., Maecke H.R. (2011). PET of somatostatin receptor-positive tumors using 64Cu- and 68Ga-somatostatin antagonists: the chelate makes the difference. J Nucl Med.